# Dimeric Gd-tetraazacyclododecanetetraacetic acid-folate

Chemical name: | Dimeric Gd-tetraazacyclododecane-tetraacetic acid-folate
Abbreviated name: | P866
Synonym:
Agent category: | Compound
Target: | Folate receptor
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P866)]

Folic acid (folate) is a water-soluble B vitamin (1) essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is with the facilitated transporter folate-binding protein (FBP), which has a low affinity for folate with a K_m_ value of 1–5 μM. Some cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a high-affinity receptor (dissociation constant (K_d_), 0.5 nM) that allows folate retention via receptor-mediated endocytosis. Some human epithelial tumor cells have been found to overexpress FBP (2). More than 90% of human ovarian and endometrial cancers express the high-affinity folate receptor, which is absent in normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the folate receptor but to a lesser frequency (20–50%).

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (3, 4). Gd-Labeled diethylenetriaminepentaacetic acid (Gd-DTPA) was the first intravenous magnetic resonance imaging (MRI) contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancer; furthermore, they are largely nonspecific. P866 is composed of folic acid coupled to a high-relaxivity dimeric Gd-tetraazacyclododecane-tetraacetic acid (Gd-DOTA) derivative. P866 has been studied as a MRI agent for folate receptor expression in nude mice bearing human cancer xenografts and in rats with arthritis (5-7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P866+synthesis)]

P866 is commercially available (Guerbet Research, Paris, France) and has a molecular weight of 9.4 kDa with two Gd-DOTA moieties and one folic acid molecule per P866 molecule (7). P1001 is composed of the two Gd-DOTA moieties without folic acid. The r1 and r2 relaxivities of P866 and P1001 are ~21 and ~30 mmol^-1^s^-1^ in water at 60 MHz and 37°C, respectively. On the other hand, the r1 and r2 relaxivities of Gd-DOTA are 3.1 and 3.7 mmol^-1^s^-1^ in water at 60 MHz and 37°C, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P866+in+vitro)]

Corot et al. (6) performed binding experiments with P866 and folic acid with use of a Biacore sensor chip immobilized with FPB. The K_d_ value of P866 was calculated to be 26.7 µM, and the K_d_ value of folic acid was 10.0 µM. Using in vitro binding experiments on KB tumor cells, [^3^H]folic acid bound to a single site with a K_d_ value of 0.9 nM and a maximal binding value of 7 million folate receptor binding sites/cell. The 50% inhibition concentration values were 5.9 and 59.3 nM for folic acid and P866, respectively. After incubation of 80 uM P866 on KB tumor cells for 2 h, the r1 relaxivity for tumor cells was 19.6 mmol^-1^s^-1^, which was 22% lower than that for tumor cells alone. Co-incubation with excess folic acid abrogated the change in the r1 relaxivity induced by P866 as well as the reduction of Gd concentration in the KB cells by ~90%. HT1080 (negative for the folate receptor) tumor cells showed little change in the r1 relaxivity after incubation with P866.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P866+rodentia)]

Using an antigen-induced arthritis model in rats (n = 15), Saborowski et al. (7) showed that T1 relaxation times of the synovitis at 2 h after injection with P866 (0.02 mmol/kg) was significantly shortened (P < 0.05) with little change in T1 relaxation times in the normal joint. On the other hand, injection with P1001 (0.02 mmol/kg) or Gd-DOTA (0.01 mmol/kg) induced little change in T1 relaxation times in the synovitis. The blood half-lives were 19.4, 28.8, and 31.0 min for P866, P1001, and Gd-DOTA, respectively. Autoradiography studies of tissue sections showed a four-fold higher amount of folate receptor in the arthritic joint as compared with the normal joint. Histoimmunological staining showed that infiltrating lymphocytes and macrophages in the arthritic joint were positive for folate receptors.

Corot et al. (6) performed 2.4-T MRI studies for 4 h in mice bearing human KB tumor xenografts with 0.015 mmol/kg P866 and P1001. There was a significant increase (P < 0.05) in tumor T1w maximum enhancement in the KB tumors for P866 (n = 7 mice, 42 ± 18%) over P1001 (n = 6 mice, 25 ± 14%). Biodistribution studies were also performed (n = 3 mice/group) at 1, 4, and 24 h after injection, with tumor Gd levels of 3.2, 2.7, and 2.1% injected dose/g, respectively. The tumor/muscle ratios were 2.2, 5.1, and 4.0 at 1, 4, and 24 h after injection, respectively. Co-administration of folic acid (0.1 mmol/kg) inhibited the binding by 27, 49, and 49% at 1, 4, and 24 h after injection, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P866+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P866+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P866+human)]

No publication is currently available.

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
4 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
5 Wang Z.J., Boddington S., Wendland M., Meier R., Corot C., Daldrup-Link H. (2008). MR imaging of ovarian tumors using folate-receptor-targeted contrast agents. Pediatr Radiol.
6 Corot C., Robert P., Lancelot E., Prigent P., Ballet S., Guilbert I., Raynaud J.S., Raynal I., Port M. (2008). Tumor imaging using P866, a high-relaxivity gadolinium chelate designed for folate receptor targeting. Magn Reson Med.
7 Saborowski O., Simon G.H., Raatschen H.J., Wendland M.F., Fu Y., Henning T., Baehner R., Corot C., Chen M.H., Daldrup-Link H.E. (2007). MR imaging of antigen-induced arthritis with a new, folate receptor-targeted contrast agent. Contrast Media Mol Imaging.